# IRDye800CW-anti-CD105 TRC105 chimeric monoclonal antibody

Chemical name: | IRDye800CW-anti-CD105 TRC105 chimeric monoclonal antibody
Abbreviated name: | IRDye800CW-TRC105
Synonym:
Agent category: | Antibody
Target: | CD105 (Endoglin, EDG)
Target category: | Antigen
Method of detection: | Optical, near-infrared (NIR) fluorescence
Source of signal/ contrast: | IRDye 800CW
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4557555), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=10862690) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2022) for more information about CD105

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=TRC105)]

Angiogenesis is an essential process in the development of new blood vessels both in normal physiological states and diseases (1, 2). Targeting of tumor vasculature is a promising strategy for tumor imaging and therapy because tumor growth and metastasis largely depend on angiogenesis (3-5). Transforming growth factor-β (TGF-β) is a pleiotropic cytokine that modulates blood vessel development, angiogenesis, and tumor progression (6). There are three isoforms of TGF-β (β_1_, β_2_, and β_3_). TGF-β_1_ inhibits proliferation and migration of endothelial cells and their ability to form capillaries. CD105 (endoglin, EDG) is a homodimeric transmembrane glycoprotein (180 kDa) with disulfide-linked subunits of 95,000. CD105 is a component of the TGF-β receptor complex that specifically binds TGF-β_1_ and TGF-β_3_ with high affinity (7). CD105 is important for blood vessel development. The expression of CD105 on different cells affects cellular response to TGF-β_1_. CD105 is overexpressed in proliferating endothelial cells of tumor vessels, and CD105 prevents TGF-β_1_–mediated inhibition of endothelial cell proliferation (8, 9).

Radiolabeled monoclonal antibodies (mAbs) have been developed for both the diagnosis and treatment of tumors (10-12). Quiescent human endothelial cells express CD105 only weakly, but the expression of CD105 is strongly upregulated on the endothelial cells of tumor tissues undergoing angiogenesis (9, 13). The high level of expressed CD105 (up to 10^6^ molecules/proliferating cell) appears to be ideal for in vivo imaging and therapy. Anti-CD105 mAbs, such as MAEND3, E9, and MJ7/18 with radioisotopes (e.g., ^111^In, ^99m^Tc, and ^125^I) have been studied as single-photon emission computed tomography (SPECT) probes for imaging CD105 expression (9, 14). TRC105 is a human/murine chimeric IgG_1_ mAb that binds with higher affinity to human CD105 than to murine CD105 (15). TRC105 inhibits angiogenesis and tumor growth and is now in clinical trials in cancer patients. Binding of TRC105 to CD105 allows TGF-β_1_–mediated inhibition of endothelial cell proliferation. Hong et al. (16) showed that ^64^Cu-1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid-anti-CD105 TRC105 (^64^Cu-DOTA-TRC105) mAb could efficiently image 4T1 murine breast tumor in mice with positron emission tomography (PET) imaging. Hong et al. (17) have evaluated ^89^Zr-desferrioxamine-TRC105 (^89^Zr-Df-TRC105) as an ^89^Zr-based PET agent in the same 4T1 murine breast tumor model. For near-infrared (NIR) fluorescence optical imaging, Yang et al. (18) conjugated IRDye800CW to TRC105 to form IRDye800CW-TRC105 to assess CD105 expression in mice bearing 4T1 murine breast tumors.

### Related Resource Links:

- Chapters in MICAD (CD105 (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=(CD105%20OR%20endoglin)+AND+micad%5Bbook%5D))
- Gene information in NCBI (CD105 (http://www.ncbi.nlm.nih.gov/gene/2022), TGF-β_1_ (http://www.ncbi.nlm.nih.gov/gene/7040))
- Articles in Online Mendelian Inheritance in Man (OMIM) (CD105 (http://www.ncbi.nlm.nih.gov/omim/131195), TGF-β_1_ (http://omim.org/entry/190180?search=tgf&highlight=tgf))
- Clinical trials (TRC105 (http://www.clinicaltrials.gov/ct2/results?term=TRC105))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=TRC105+AND+synthesis)]

Commercially available IRDye800CW-N-hydroxysuccinimide ester (LI-COR, Lincoln, NE) was used to conjugate TRC105 in 1:1 molar ratio to form IRDye800CW-TRC105, which was purified with column chromatography (18). The molar ratio of IRDye800CW to TRC105 in the conjugated antibody was 0.4 with >85% yield. IRDye800CW-cetuximab was also prepared similarly as an isotype-matched control with a similar number of dye molecules per antibody. Cetuximab is an anti-EGFR mouse-human chimeric IgG_1_ mAb.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=TRC105+AND+in+vitro)]

Yang et al. (18) performed in vitro indirect fluorescence staining with unlabeled TRC105 and IRDye800CW-TRC105 on MCF7 human breast cancer cells (CD105-negative) and human umbilical vein endothelial cells (HUVECs, CD105-positive). Fluorescence microscopy and flow cytometry showed strong CD105 expression in HUVECs but weak or no expression in MCF7 cells. No significant differences in fluorescence intensities between TRC105 and IRDye800CW-TRC105 were observed in the HUVEC cells, suggesting that IRDye800CW-TRC105 retains immunoreactivity similar to that of the unconjugated mAb.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=TRC105+AND+in+vitro)]

Yang et al. (18) studied the accumulation of IRDye800CW-TRC105 using a whole-body fluorescence detection system in mice bearing CD105-positive 4T1 tumors. IRDye800CW-TRC105 (0.3 nmol/mouse) was injected intravenously into mice (n = 3) that showed distinct fluorescence signals in the tumors at 0.5–48 h after injection with a plateau at ~16 h. Regions of interest analysis showed tumor signal levels of 1.91, 1.98, 2.63, 3.70, 5.11, 4.86, and 4.94 × 10^4^ counts/s per mm^2^ at 0.5, 1, 2, 4, 16, 24, and 48 h after injection, respectively. Pretreatment with TRC105 (13 nmol/mouse, time of pretreatment not reported) significantly (P < 0.05) inhibited the IRDye800CW-TRC105 binding in the tumors by >50% at each time point starting 1 h after injection. IRDye800CW-cetuximab showed tumor signal levels of 0.68, 0.79, 1.29, 1.69, 4.00, 4.23, and 4.37 × 10^4^ counts/s per mm^2^ at 0.5, 1, 2, 4, 16, 24, and 48 h after injection, respectively. The signals levels of IRDye800CW-cetuximab were lower than those of IRDye800CW-TRC105 at all the time points. The passive accumulation of IRDye800CW-cetuximab at the later time points may be due to the longer circulation half-life of cetuximab (11.5 h) than that of TRC105 (3.5 h). In comparison, IRDye800CW showed significantly (P < 0.05) lower tumor fluorescence signal than IRDye800CW-TRC105 and IRDye800CW-cetuximab at 4–48 h.

Ex vivo NIR fluorescence imaging was performed at 48 h after injection (18). There was a prominent accumulation of IRDye800CW-TRC105 in the liver with some detectable accumulation in the kidneys. The accumulation in tumor was higher than in other major organs except the liver, and accumulation was blocked by pretreatment with TRC105. On the other hand, IRDye800CW-cetuximab exhibited fluorescence signal only in the liver and tumor. The tumor signal was only ~33% of the signal with IRDye800CW-TRC105. Immunofluorescence staining of 4T1 tumor sections showed colocalization of CD31 with CD105 on the tumor endothelial cells (CD31- and CD105-positive) but not on tumor cells (CD31-negative, CD105-positive). On the other hand, there was only a weak CD105 staining on the liver and spleen sections.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=TRC105+AND+(dog+OR+rabbit+OR+pig+OR+sheep))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=TRC105+AND+(primate+NOT+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=TRC105+AND+human)]

No publication is currently available.

## References

1 Carmeliet P., Jain R.K. (2011). Molecular mechanisms and clinical applications of angiogenesis. Nature.
2 Folkman J. (1995). Angiogenesis in cancer, vascular, rheumatoid and other disease. Nat Med.
3 Fonsatti E., Altomonte M., Arslan P., Maio M. (2003). Endoglin (CD105): a target for anti-angiogenetic cancer therapy. Curr Drug Targets.
4 Abdollahi A., Folkman J. (2010). Evading tumor evasion: current concepts and perspectives of anti-angiogenic cancer therapy. Drug Resist Updat.
5 Thorpe P.E. (2004). Vascular targeting agents as cancer therapeutics. Clin Cancer Res.
6 Massague J., Cheifetz S., Laiho M., Ralph D.A., Weis F.M., Zentella A. (1992). Transforming growth factor-beta. Cancer Surv.
7 Cheifetz S., Bellon T., Cales C., Vera S., Bernabeu C., Massague J., Letarte M. (1992). Endoglin is a component of the transforming growth factor-beta receptor system in human endothelial cells. J Biol Chem.
8 Tabata M., Kondo M., Haruta Y., Seon B.K. (1999). Antiangiogenic radioimmunotherapy of human solid tumors in SCID mice using (125)I-labeled anti-endoglin monoclonal antibodies. Int J Cancer.
9 Bredow S., Lewin M., Hofmann B., Marecos E., Weissleder R. (2000). Imaging of tumour neovasculature by targeting the TGF-beta binding receptor endoglin. Eur J Cancer.
10 Wu A.M., Senter P.D. (2005). Arming antibodies: prospects and challenges for immunoconjugates. Nat Biotechnol.
11 Milenic D.E., Brechbiel M.W. (2004). Targeting of radio-isotopes for cancer therapy. Cancer Biol Ther.
12 Kowalsky, R.J., S.W. Falen, Radiopharmaceutcals in nuclear pharmacy and nuclear medicine. Second ed. 2004, Washington, D.C.: APhA. 733-752.
13 Seon B.K., Haba A., Matsuno F., Takahashi N., Tsujie M., She X., Harada N., Uneda S., Tsujie T., Toi H., Tsai H., Haruta Y. (2011). Endoglin-targeted cancer therapy. Curr Drug Deliv.
14 Fonsatti E., Jekunen A.P., Kairemo K.J., Coral S., Snellman M., Nicotra M.R., Natali P.G., Altomonte M., Maio M. (2000). Endoglin is a suitable target for efficient imaging of solid tumors: in vivo evidence in a canine mammary carcinoma model. Clin Cancer Res.
15 Tsujie M., Tsujie T., Toi H., Uneda S., Shiozaki K., Tsai H., Seon B.K. (2008). Anti-tumor activity of an anti-endoglin monoclonal antibody is enhanced in immunocompetent mice. Int J Cancer.
16 Hong H., Yang Y., Zhang Y., Engle J.W., Barnhart T.E., Nickles R.J., Leigh B.R., Cai W. (2011). Positron emission tomography imaging of CD105 expression during tumor angiogenesis. Eur J Nucl Med Mol Imaging.
17 Hong, H., G.W. Severin, Y. Yang, J.W. Engle, Y. Zhang, T.E. Barnhart, G. Liu, B.R. Leigh, R.J. Nickles, and W. Cai, Positron emission tomography imaging of CD105 expression with (89)Zr-Df-TRC105. Eur J Nucl Med Mol Imaging, 2011
18 Yang Y., Zhang Y., Hong H., Liu G., Leigh B.R., Cai W. (2011). In vivo near-infrared fluorescence imaging of CD105 expression during tumor angiogenesis. Eur J Nucl Med Mol Imaging.